# [^11^C]N,N-Dimethyl-2-(2-amino-4-cyanophenylthio)benzylamine

Chemical name: | [^11^C]N,N-Dimethyl-2-(2-amino-4-cyanophenylthio)benzylamine
Abbreviated name: | [^11^C]DASB
Synonym: | [^11^C]3-Amino-4-(2-dimethylaminomethylphenylsulfanyl)-benzonitrile
Agent Category: | Compound
Target: | Serotonin transporter
Target Category: | Serotonin transporter binding
Method of detection: | PET
Source of signal\contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DASB%5BAll%20Fields%5D)]

Serotonin (5-hydroxytryptamine, 5-HT) has diverse physiological roles as a neurotransmitter in the central nervous system (1). It also is a regulator of smooth muscle function and platelet aggregation. The brain 5-HT system has been implicated in several neuropsychiatric disorders, including major depression, anxiety, obsessive-compulsive disorder, and schizophrenia (2, 3). The serotonergic transmission is controlled in part by the serotonin transporter (SERT), which regulates the concentration of free, active 5-HT in the synaptic cleft. Citalopram, paroxetine, and fluoxetine were developed as selective SERT inhibitors to treat depression and anxiety disorders by blocking the reuptake of 5-HT [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Citalopram%2C%20paroxetine%20and%20fluoxetine%20%29%20and%20human)]. The blockade led to a higher 5-HT concentration in the synaptic cleft, and subsequently an improved well-being of the patients.

Trans-1,2,3,5,6,10-β-Hexahydro-6-[4-([^11^C]methylthio)phenyl[pyrrolo-[2,1-a]isoquinoline ([^11^C]McN5652) binds selectively to the SERT, and its regional distribution of binding in humans correlates well with the known distribution of the SERT in human brain (4). However, usefulness of [^11^C]McN5652 may be limited by its nonspecific binding and slow release from specific binding sites (5). [^11^C]N,N-Dimethyl-2-(2-amino-4-cyanophenylthio)benzylamine ([^11^C]DASB) was found to be a promising tracer for SERT imaging in animals and humans (6-9). It displayed a nanomolar affinity for SERT and a greater than 1000-fold affinity for SERT over dopamine transporter (DAT) and norepinephrine transporter (NET). The uptake in the SERT-rich brain regions was both saturable and selective for SERT.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DASB%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D)]

[^11^C]DASB was synthesized by alkylation of its N-normethyl precursor using [^11^C]iodomethane in 30-55% radiochemical yield (not corrected for decay) in 25-30 min (6). Chemical and radiochemical purities were >98% with specific activities of 25-55 GBq/μmol (0.68-1.49 Ci/μmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DASB%5BAll%20Fields%5D%20AND%20in%20vitro)]

[^11^C]DASB was reported to bind specifically to the serotonergic transporter in homogenates of rat forebrain membrane (8). The transporter-binding affinity of DASB was evaluated by competitive radioaffinity assays for serotonin (SERT), norepinephrine (NET), and dopamine (DAT). Binding affinity (K_i_, nM) of DASB at SERT, NET, and DAT were 0.97, 6,000, and 1,180 nM, respectively. DASB binding selectively to SERT over other monoamine transporters was also reported previously using cloned human transporters (6). DASB inhibited selectively [^3^H]5-HT re-uptake into rat brain synaptic vesicles. K_d_, obtained from saturation data, was 0.54 nM, and B_max_ was 1.4 pmol/mg protein (10). The IC_50_ of serotonin to displace 50% of binding of 1.0 nM [^11^C]DASB was 3.47 μM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DASB%5BAll%20Fields%5D%20AND%20%28%22rodentia%22%5BMeSH%20Terms%5D%20OR%20rodentia%5BText%20Word%5D%29)]

Intravenous injection of [^11^C]DASB in rats resulted in high uptake of radioactivity in the lungs (5.99% injected dose (ID/g)) and kidneys (2.62% ID/g) at 5 min after injection (8). Less pronounced uptake was seen in the whole brain (0.79% ID/g). The uptake in the hypothalamus (0.8% ID/g), thalamus (0.64% ID/g), hippocampus (0.5% ID/g), striatum (0.55% ID/g), and cortex (0.5% ID/g) was higher than the cerebellum (0.13% ID/g) at 45 min (6). The brain regional radioactivity was blocked by pretreatment of paroxetine and fluoxetine (SERT inhibitors), except in the cerebellum, indicating that SERT is low and the cerebellum can be used as a reference region (8). The [^11^C]DASB uptake in the SERT-rich brain regions returned to >90% baseline levels in 24-48 h after paroxetine treatment. Pretreatment of rats with unlabeled DASB reduced binding of [^11^C]DASB in a dose-dependent manner. The mean ED_50_ for the whole brain is 56 nmol/kg. Elimination of [^11^C]DASB was via the hepatobiliary and renal systems.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DASB%20and%20%28pig%20or%20cat%20or%20dog%20or%20rabbit%20or%20sheep%29)]

[^11^C]DASB (200 MBq or 5.4 mCi) was injected in pigs to study its positron emission tomography (PET) imaging properties of brain SERT (11). The fraction of intact tracer in plasma at 10 min after injection was 35%. Citalopram pretreatment reduced the binding potential and distribution volume of [^11^C]DASB markedly in the mesencephalon, striatum, and frontal cortex. There was substantial agreement between results of several methods of kinetic analysis. There was a uniform displacement of 80% of [^11^C]DASB specific binding after citalopram in vivo.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DASB%20AND%20%28primate%20not%20human%29)]

In monkeys, [^11^C]DASB uptake was greatest in lungs, followed by the urinary bladder, gallbladder, brain, and other organs at 7-95 min (12). The tracer was eliminated via the hepatobiliary and renal systems. Paroxetine (SERT inhibitor) and 3,4-methylenedioxymethamphetamine (5-HT neurotoxicity) reduced the uptake of [^11^C]DASB in brain regions with high SERT density (13). The biological half-life in plasma was 30 min. The metabolism led to very polar metabolites (19% of total [^11^C]DASB radioactivity in 30 min) and one or more lipophilic metabolites in the plasma.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DASB%20and%20human)]

Nine healthy volunteers received intravenous injections of 350 MBq (9.7 mCi) [^11^C]DASB (7). Sequential images of the brain were taken over a 90-min period. The highest uptake was in the mid-brain, thalamus, hypothalamus, and striatum. The peak uptake occurred at 30-40 min. After pretreatment with an oral dose of 40 mg of citalopram, there was an 80% reduction in specific binding of [^11^C]DASB in SERT-rich regions. The metabolism of [^11^C]DASB was rapid, with about 50% of the intact compound remaining in plasma at 20 min after injection.

No difference in regional SERT binding potential was found between major depressive episodes and normal subjects as measured by [^11^C]DASB PET (9). In a subgroup of patients with major depressive episodes patients and with more negativistic dysfunctional attitudes, there was a significantly higher SERT binding potential, which led to low extracellular 5-HT. It was suggested that the lower 5-HT level caused these patients to feel more negativistic. [^11^C]DASB PET is being evaluated as a useful tool for antidepressant development (14), obsessive-compulsive disorder studies (15) and alcoholism (16).

Human dosimetry of [^11^C]DASB was estimated in seven normal volunteers (17). Dynamic whole-body PET scans were acquired after the injection of 669 ± 97 MBq (18.1 ± 2.6 mCi) of [^11^C]DASB. Uptake of [^11^C]DASB in the lungs was rapid and high, with a peak of 53.1%ID within 18-46 s after injection. About 12% ID was excreted in urine. The organs that received the highest absorbed doses were found to be the lungs (0.0328 mGy/MBq or 121 mrad/mCi), the urinary bladder (0.012 mGy/MBq or 44 mrad/mCi), the kidneys (0.0093 mGy/MBq or 34 mrad/mCi), the gallbladder (0.0093 mGy/MBq or 34 mrad/mCi), and the liver (0.0064 mGy/MBq or 24 mrad/mCi). The effective dose was calculated as 0.0070 mSv/MBq (26 mrem/mCi) for a 70-kg-standard man.

## NIH Support

MH62185, MH40695, MH01997, DA05707, DA06275, AG14400, AA11653, intramural research program

## References

1 Lucki I. (1998). The spectrum of behaviors influenced by serotonin. Biol Psychiatry.
2 Abi-Dargham A., Laruelle M., Aghajanian G.K., Charney D., Krystal J. (1997). The role of serotonin in the pathophysiology and treatment of schizophrenia. J Neuropsychiatry Clin Neurosci.
3 Charney D.S. (1998). Monoamine dysfunction and the pathophysiology and treatment of depression. J Clin Psychiatry.
4 Parsey R.V., Kegeles L.S., Hwang D.R., Simpson N., Abi-Dargham A., Mawlawi O., Slifstein M., Van Heertum R.L., Mann J.J., Laruelle M. (2000). In vivo quantification of brain serotonin transporters in humans using [11C]McN 5652. J Nucl Med.
5 Szabo Z., Scheffel U., Mathews W.B., Ravert H.T., Szabo K., Kraut M., Palmon S., Ricaurte G.A., Dannals R.F. (1999). Kinetic analysis of [11C]McN5652: a serotonin transporter radioligand. J Cereb Blood Flow Metab.
6 Wilson A.A., Ginovart N., Schmidt M., Meyer J.H., Threlkeld P.G., Houle S. (2000). Novel radiotracers for imaging the serotonin transporter by positron emission tomography: synthesis, radiosynthesis, and in vitro and ex vivo evaluation of (11)C-labeled 2-(phenylthio)araalkylamines. J Med Chem.
7 Houle S., Ginovart N., Hussey D., Meyer J.H., Wilson A.A. (2000). Imaging the serotonin transporter with positron emission tomography: initial human studies with [11C]DAPP and [11C]DASB. Eur J Nucl Med.
8 Wilson A.A., Ginovart N., Hussey D., Meyer J., Houle S. (2002). In vitro and in vivo characterisation of [11C]-DASB: a probe for in vivo measurements of the serotonin transporter by positron emission tomography. Nucl Med Biol.
9 Meyer J.H., Houle S., Sagrati S., Carella A., Hussey D.F., Ginovart N., Goulding V., Kennedy J., Wilson A.A. (2004). Brain serotonin transporter binding potential measured with carbon 11-labeled DASB positron emission tomography: effects of major depressive episodes and severity of dysfunctional attitudes. Arch Gen Psychiatry.
10 Lundquist P., Wilking H., Hoglund A.U., Sandell J., Bergstrom M., Hartvig P., Langstrom B. (2005). Potential of [(11)C]DASB for measuring endogenous serotonin with PET: binding studies. Nucl Med Biol.
11 Jensen S.B., Smith D.F., Bender D., Jakobsen S., Peters D., Nielsen E.O., Olsen G.M., Scheel-Kruger J., Wilson A., Cumming P. (2003). [11C]-NS 4194 versus [11C]-DASB for PET imaging of serotonin transporters in living porcine brain. Synapse.
12 Belanger M.J., Simpson N.R., Wang T., Van Heertum R.L., Mann J.J., Parsey R.V. (2004). Biodistribution and radiation dosimetry of [11C]DASB in baboons. Nucl Med Biol.
13 Szabo Z., McCann U.D., Wilson A.A., Scheffel U., Owonikoko T., Mathews W.B., Ravert H.T., Hilton J., Dannals R.F., Ricaurte G.A. (2002). Comparison of (+)-(11)C-McN5652 and (11)C-DASB as serotonin transporter radioligands under various experimental conditions. J Nucl Med.
14 Meyer J.H. (2007). Imaging the serotonin transporter during major depressive disorder and antidepressant treatment. J Psychiatry Neurosci.
15 Reimold M., Smolka M.N., Zimmer A., Batra A., Knobel A., Solbach C., Mundt A., Smoltczyk H.U., Goldman D., Mann K., Reischl G., Machulla H.J., Bares R., Heinz A. (2007). Reduced availability of serotonin transporters in obsessive-compulsive disorder correlates with symptom severity - a [11C]DASB PET study. J Neural Transm.
16 Brown A.K., George D.T., Fujita M., Liow J.S., Ichise M., Hibbeln J., Ghose S., Sangare J., Hommer D., Innis R.B. (2007). PET [11C]DASB imaging of serotonin transporters in patients with alcoholism. Alcohol Clin Exp Res.
17 Lu J.Q., Ichise M., Liow J.S., Ghose S., Vines D., Innis R.B. (2004). Biodistribution and radiation dosimetry of the serotonin transporter ligand 11C-DASB determined from human whole-body PET. J Nucl Med.